# ^99m^Tc-(3Z)-4-{4-[2-(Dimethylamino)ethoxy]phenyl}-3,4-diphenylbut-3-en-1-ylN,N-bis[2-(2,6-dioxomorpholin-4-yl)ethyl]glycinate

Chemical name: | ^99m^Tc-(3Z)-4-{4-[2-(Dimethylamino)ethoxy]phenyl}-3,4-diphenylbut-3-en-1-ylN,N-bis[2-(2,6-dioxomorpholin-4-yl)ethyl]glycinate
Abbreviated name: | ^99m^Tc-DTPA-TOR, ^99m^Tc-TOR-DTPA
Synonym:
Agent category: | Compound
Target: | Estrogen receptor
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA)]

Estrogens and progestins are endogenous hormones that produce many physiological effects (1). Estrogens act primarily by regulating gene expression. Estrogen receptors (ERs) are found in the cytoplasm and nucleus of cells of the female reproductive tract, breast, pituitary, hypothalamus, bone, liver, and other tissues, and also in various tissues in men. Estrogens are lipophilic in that they enter the cell passively by diffusion through the cellular membrane. Estrogens bind to ERs that are present in the cytoplasm and the complexes are transported into the nucleus.

Breast cancer is the most common malignancy in women. Approximately 33% of women who have this disease will die of disseminated breast cancer. The growth of breast epithelial cells is dependent on estrogen stimulation, which induces progestin receptor expression. Two thirds of breast carcinomas express ERs. It has also been established that the ER status of the tumor is an important prognostic indicator in breast cancer (2). Women with ER-positive breast tumors have a better prognosis than women with ER-negative tumors in terms of responsiveness to anti-estrogen treatment. ER content in breast cancer is assessed in vitro with receptor binding assays, which suffer from interassay variability, are limited by intrinsic receptor heterogeneity of the tumor, and do not yield information on the ER density in metastases. 16α-[^18^F]Fluoro-17β-estradiol ([^18^F]FES) has been proven to be a valuable tracer for studies of the ER status of primary and metastatic breast cancer (3). However, [^18^F]FES was cleared from the blood and was metabolized in 20 min with only 20% of [^18^F]FES intact in a study of 15 breast cancer patients (4). Toremifene (TOR) is a chlorinated analog of tamoxifen (5, 6), which was first approved by the United States Food and Drug Administration (http://www.fda.gov/ohrms/dockets/ac/06/briefing/2006-4248B1-01-FDA-Tamoxifen Background Summary Final.pdf) in the 1970s for use in breast cancer treatment. TOR is primarily used in the treatment of patients with metastatic breast cancer (7). Yurt et al. (8) coupled diethylenetriamine pentaacetic acid (DTPA) to TOR to form (3Z)-4-{4-[2-(dimethylamino)ethoxy]phenyl}-3,4-diphenylbut-3-en-1-ylN,N-bis[2-(2,6-dioxomorpholin-4-yl)ethyl]glycinate (DTPA-TOR) and radiolabeled the DTPA-TOR with ^99m^Tc. ^99m^Tc-DTPA-TOR exhibited high breast tissue/background ratio in female rats.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=estrogen%20receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Estrogen receptor (http://www.ncbi.nlm.nih.gov/gene/2099))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=133430)
- Clinical trials (Toremifene (http://www.clinicaltrials.gov/ct2/results?term=Toremifene))
- Drug information in FDA (http://google2.fda.gov/search?q=Toremifene&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=8)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA%20AND%20synthesis)]

Yurt et al. (8) reported the radiolabeling of DTPA-TOR with ^99m^Tc. DTPA-anhydride (0.12 mmol) was added to a solution of TOR (0.05 mmol) in acetone to produce DTPA-TOR. Mass spectroscopy showed that the agents bound in a ratio of one DTPA per TOR. The mixture was incubated for 12 h at room temperature. DTPA-TOR (0.1 mg) was mixed with 740 MBq (20 mCi) ^99m^TcO_4_^-^ and SnCl_2_ (0.1 mg). The mixture was incubated for 25 min at room temperature. The ^99m^Tc-labeling efficiency was ~80%, and the specific activity was ~15 MBq/nmol (0.4 mCi/nmol) at the time of injection.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA%20AND%20in%20vitro)]

^99m^Tc-DTPA-TOR exhibited an experimental log P value of -2.04 at pH 7.0 (8). ^99m^Tc-DTPA-TOR was intact in human serum for up to 60 min of incubation at 37°C and was ~45% intact after 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA%20AND%20rodentia)]

It was demonstrated that ^99m^Tc-DTPA-TOR accumulation by target tissue (breast) in young female rats (n = 3/group) is highly specific (8). Rats were injected with ~30 MBq (0.8 mCi (5.7 nmol)) ^99m^Tc-DTPA-TOR. The tissue accumulations were expressed as tissue/muscle ratios. The breast/muscle ratios were 1.6, 8.5, and 13.2 at 30, 60, and 240 min after injection, respectively. The ovary/muscle and uterus/muscle ratios were 3.9 and 3.3 at 240 min, respectively. The stomach (130.4), kidney (16.7), intestines (21.7–29.8), and urinary bladder (32.2) exhibited high tissue/muscle ratios at 240 min after injection. Pretreatment with 10-fold excess DTPA-TOR (57 nmol) showed significant inhibition (P < 0.05) of the breast/muscle ratios (88% at 60 min and 68% at 240 min after injection). However, little inhibition was observed in the uterus and ovary.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA%20AND%20primates%20not%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TOR-DTPA%20AND%20human)]

No publication is currently available.

## References

1 Beato M., Klug J. (2000). Steroid hormone receptors: an update. Hum Reprod Update.
2 Vollenweider-Zerargui L., Barrelet L., Wong Y., Lemarchand-Beraud T., Gomez F. (1986). The predictive value of estrogen and progesterone receptors' concentrations on the clinical behavior of breast cancer in women. Clinical correlation on 547 patients. Cancer.
3 Flanagan F.L., Dehdashti F., Siegel B.A. (1998). PET in breast cancer. Semin Nucl Med.
4 Mankoff D.A., Tewson T.J., Eary J.F. (1997). Analysis of blood clearance and labeled metabolites for the estrogen receptor tracer [F-18]-16 alpha-fluoroestradiol (FES). Nucl Med Biol.
5 da Costa G.G., Pereira P.C., Churchwell M.I., Beland F.A., Marques M.M. (2007). DNA adduct formation in the livers of female Sprague-Dawley rats treated with toremifene or alpha-hydroxytoremifene. Chem Res Toxicol.
6 Kim S.Y., Suzuki N., Santosh Laxmi Y.R., Rieger R., Shibutani S. (2003). Alpha-hydroxylation of tamoxifen and toremifene by human and rat cytochrome P450 3A subfamily enzymes. Chem Res Toxicol.
7 Saeki T., Okita A., Aogi K., Kakishita T., Okita R., Taira N., Ohama Y., Takashima S., Nishikawa K. (2009). Pharmacokinetic analysis of a combined chemoendocrine treatment with paclitaxel and toremifene for metastatic breast cancer. Breast Cancer.
8 Yurt A., Muftuler F.Z., Unak P., Yolcular S., Acar C., Enginar H. (2009). Synthesis of a novel antiestrogen radioligand (99mTc-TOR-DTPA). Cancer Biother Radiopharm.
9 Federici L., Blondet C., Imperiale A., Sibilia J., Pasquali J.L., Pflumio F., Goichot B., Blaison G., Weber J.C., Christmann D., Constantinesco A., Andres E. Value of (18)F-FDG-PET/CT in patients with fever of unknown origin and unexplained prolonged inflammatory syndrome: a single centre analysis experience. Int J Clin Pract.